# Anti-c-Met monoclonal antibody linked to biotinylated bovine serum albumin and gadolinium

Chemical name: | Anti-c-Met monoclonal antibody linked to biotinylated bovine serum albumin and gadolinium
Abbreviated name: | Anti-c-Met-Gd-albumin
Synonym:
Agent Category: | Biotinylated bovine serum albumin
Target: | Tyrosine kinase receptor c-Met
Target Category: | Binding
Method of detection: | Magnetic resonance imaging (MRI)
Source of Signal/Contrast: | Gadolinium
Activation: | No
Studies: | - In vitro; - Rodents | Structure of anti-c-Met-Gd-albumin not available.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=anti+c+Met+Gd+albumin)]

Gliomas and glioblastoma multiforme are characterized as highly infiltrative and invasive forms of brain cancer that may be treated with either surgical resection, chemotherapy, radiotherapy, or a combination of these modalities (1). However, with a median survival time of less than 18 months, the prognosis for the patient is poor regardless of the option used to treat this cancer (2). The tyrosine kinase receptor c-Met plays an important role in invasive cell growth and motility during embryogenesis and is a tumor marker for several cancers including gliomas (3, 4). c-Met is a transmembrane glycoprotein (Mw = 190 kD) that consists of a β subunit and an extracellular α subunit that binds and is activated by the hepatocyte growth factor (HGF) (5). For individuals with malignant meningiomas, overexpression of HGF correlates with a poor prognosis, and this factor has also been used to predict tumor recurrence (6). Because of their role in the development of brain tumors, both c-Met and HGF are considered important markers to predict angiogenesis and tumor growth (7). Several clinical trials (http://clinicaltrials.gov/ct2/results?term=glioma) are in progress to develop suitable treatment(s) for these brain tumors.

Towner et al. envisioned that early detection of glioma tumors would perhaps improve treatment outcomes for the patients (8). They used an anti-c-Met monoclonal antibody (MAb) linked to gadolinium (through diethylenetriaminepentaacetic acid (DTPA)) and biotinylated bovine serum albumin (anti-c-Met-Gd-biotinylated BSA) to specifically target c-Met. The MAb linked to the contrast agent (CA) was then used to visualize the glioma tumors with magnetic resonance imaging (MRI) in rats bearing C6 cell glioma tumors in the brain. Biotinylated BSA was also used to facilitate detection of the CA with fluorescence staining of cryosections of brain tissue (8).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=anti+cMet+Gd+albumin+synthesis)]

The commercially available MAb used for this study was directed toward the extracellular β chain of the c-Met antigen (8).

Synthesis of the MRI CA was performed as described by Towner et al. (8). Biotinylation of the BSA was performed using a modification of the method of Dafni et al. (9). The conjugation of DTPA to biotinylated BSA was done in Hepes buffer (pH 8.8) by the addition of small amounts of DTPA suspended in dimethyl sulfoxide at room temperature, followed by adjustment of the reaction mixture with sodium hydroxide to pH 8.5. The mixture was stirred for 2 h at 4°C. The product was dialyzed against several changes of citrate buffer (pH 6.5), and gadolinium(III) chloride in acetate buffer (pH 6.0) was gradually added to the dialyzed compound. The mixture was incubated for 24 h at 4°C, and the resultant product, biotin-BSA-Gd-DTPA, was dialyzed against citrate buffer (pH 6.5) and double-distilled water. Biotin-BSA-Gd-DTPA was then freeze-dried and stored until required (storage conditions were not provided).

The anti-c-Met MAb was linked to biotin-BSA-Gd-DTPA through an N-hydroxysulfosuccinimide (sulfo-NHS) and 1-ethyl-3-[3-dimethylamino-propyl]carbodiimide hydrochloride (EDC) link between the MAb and the biotinylated BSA using the Hermanson's method (10). To obtain anti-c-Met-biotin-BSA-Gd-DTPA, the sulfo-NHS was reacted with EDC for 15 min at room temperature, and a solution of the anti-Met MAb was added to the mixture. The reaction proceeded for 2 h at room temperature in the dark. The final product, anti-c-Met-biotin-BSA-Gd-DTPA, was freeze-dried and stored at 4°C until required. The number of biotin and Gd-DTPA molecules linked to the BSA was not reported (8).

For use as a control, commercially available normal rat IgG was linked to biotin-BSA-Gd-DTPA as detailed above (8). The purity and stability of the various CA prepared and used in the reported studies was not reported (8).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=c+Met+biotin+BSA+Gd+DTPA+in+vitro)]

Towner et al. used indirect immunofluorescence to confirm the overexpression of c-Met in rat glioma tissue compared with normal brain tissue (8). Cryosections of the brain tissue were incubated with a rabbit anti-c-Met antibody, followed by treatment with a donkey anti-rabbit IgI-Cy3 antibody in phosphate-buffered saline. Glioma and normal tissue were also obtained from animals treated in vivo with anti-c-Met-biotin-BSA-Gd-DTPA, IgG-biotin-BSA-Gd-DTPA, or biotin-BSA-Gd-DTPA. The various tissues were then stained with streptavidin-labeled IgG linked to the Cy3 fluorescent dye. The stained sections were viewed under a confocal laser-scanning microscope. Compared with the normal tissue immunofluorescence, an enhanced signal was detected only in the glioma tissue, indicating an overexpression of c-Met in these cells. This observation was confirmed with histological immunofluorescence of brain tissue obtained after MRI of animals 3 h after treatment with the anti-c-Met-biotin-BSA-Gd-DTPA or anti-IgG-biotin-BSA-Gd-DTPA antibodies, or with biotin-BSA-Gd-DTPA, respectively, as described above (8).

Presence of higher levels of c-Met in the glioma tissues, compared with normal tissues, was confirmed with Western blot analysis (8).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=c+Met+biotin+BSA+Gd+DTPA+rodentia)]

Rats (the number of animals was not specified) were injected intravenously with the biotin-BSA-Gd-DTPA linked with or without the anti-c-Met MAb, and T_1_- and T_2_-weighted MRI imaging was performed 3 h after the treatment (8). The parameters used for MRI were: multi-slice spin echo repetition time (TR) was 2.4 s, and the echo times were 17.4 ms for the T_1_-weighted images and 63.9 ms for the T_2_-weighted images with a 128 × 128 matrix, four steps per acquisition, 3.5 × 3.5 cm^2^ field view, and a slice thickness of 1 mm. The T_2_ images provided anatomical details of the tumor locations, and the T_1_ images detected the Gd-based MAb probe in the glioma tissues. After administration of anti-c-Met-biotin-BSA-Gd-DTPA, compared with the normal brain tissue, a substantial decrease in the T_1_ value was reported in the tumor regions with a corresponding increase in the MRI signal intensity. The control tissue, from animals treated either with anti-IgG-biotin-BSA-Gd-DTPA or biotin-BSA-Gd-DTPA, respectively, showed little change in the T_1_ value or the MRI signal. Also, on the basis of the T_1_ values, the anti-c-Met CA was present in the glioma tissue even after 3 h, but the control CA showed a return to pre-contrast values during this period. No competition studies were reported.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=anti+c+Met+biotinylated+BSA+Gd+DTPA+non%2Dprimate+mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=anti+c+Met+biotinylated+BSA+Gd+DTPA+non+human+primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=anti+c+Met+biotinylated+BSA+Gd+DTPA+humans)]

No references are currently available.

## Supplemental Information

[Disclaimers]

## NIH Support

Supported by National Institutes of Health grant number 5R03CA121359-2.

## References

1 Pouratian N., Asthagiri A., Jagannathan J., Shaffrey M.E., Schiff D. (2007). Surgery Insight: the role of surgery in the management of low-grade gliomas. Nat Clin Pract Neurol.
2 Mitchell P., Ellison D.W., Mendelow A.D. (2005). Surgery for malignant gliomas: mechanistic reasoning and slippery statistics. Lancet Neurol.
3 Gentile A., Trusolino L., Comoglio P.M. (2008). The Met tyrosine kinase receptor in development and cancer. Cancer Metastasis Rev.
4 Zucali P.A., Ruiz M.G., Giovannetti E., Destro A., Varella-Garcia M., Floor K., Ceresoli G.L., Rodriguez J.A., Garassino I., Comoglio P., Roncalli M., Santoro A., Giaccone G. (2008). Role of cMET expression in non-small-cell lung cancer patients treated with EGFR tyrosine kinase inhibitors. Ann Oncol.
5 Comoglio P.M., Giordano S., Trusolino L. (2008). Drug development of MET inhibitors: targeting oncogene addiction and expedience. Nat Rev Drug Discov.
6 Arrieta O., Garcia E., Guevara P., Garcia-Navarrete R., Ondarza R., Rembao D., Sotelo J. (2002). Hepatocyte growth factor is associated with poor prognosis of malignant gliomas and is a predictor for recurrence of meningioma. Cancer.
7 Abounader R., Laterra J. (2005). Scatter factor/hepatocyte growth factor in brain tumor growth and angiogenesis. Neuro Oncol.
8 Towner R.A., Smith N., Doblas S., Tesiram Y., Garteiser P., Saunders D., Cranford R., Silasi-Mansat R., Herlea O., Ivanciu L., Wu D., Lupu F. (2008). In vivo detection of c-Met expression in a rat C6 glioma model. J Cell Mol Med.
9 Dafni H., Landsman L., Schechter B., Kohen F., Neeman M. (2002). MRI and fluorescence microscopy of the acute vascular response to VEGF165: vasodilation, hyper-permeability and lymphatic uptake, followed by rapid inactivation of the growth factor. NMR Biomed.
10 Hermanson, G., Bioconjugate Techniques1996, New York: Academic Press. p176.